# ^111^In-Diethylenetriamine pentaacetic acid-NAVPNLRGDLQVLAQKVART

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-NAVPNLRGDLQVLAQKVART
Abbreviated name: | ^111^In-DTPA-A20FMDV2
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_6_
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A20FMDV2)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_ and α_v_β_6_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

The α_v_β_6_ integrin plays an important role in the development of epithelial cells and is nearly undetectable on normal adult tissues. However, the levels of α_v_β_6_ integrin can be upregulated during tissue remodeling and wound healing (11). On the other hand, α_v_β_6_ integrin is strongly expressed on tumor cells of the oral cavity, pancreas, breast, ovary, colon, and stomach (12-14). α_v_β_6_ integrin affects tumor growth, tumor invasiveness, and metastasis (13). α_v_β_6_ binds to the RGD motif in fibronectin, tenascin, and the viral protein 1 (VP1) of the foot-and-mouth disease virus (FMDV) (15). FMDV binds to cells through the RGD motif of the GH loop of the VP1. The consensus α_v_β_6_-binding motif DLXXL was identified with the use of phage display screening, with minimal binding to α_v_β_3_, α_IIb_β_3_, and α_v_β_5_ (16). A 20-amino acid peptide, NAVPNLRGDLQVLAQKVART (A20FMDV2), was identified as a ligand binding to α_v_β_6_ integrin (15). A20FMDV2 was radiolabeled with N-succinimidyl 4-[^18^F]fluorobenzoate ([^18^F]SFB) to study in vivo biodistribution of the tracer in tumor-bearing mice (17). [^18^F]FB-A20FMDV2 (http://www.ncbi.nlm.nih.gov/books/NBK23374/) was found to have specific accumulation in α_v_β_6_-positive tumors. For single-photon emission computed tomography (SPECT), Saha et al. (18) prepared ^111^In-diethylenetriamine pentaacetic acid-A20FMDV2 (^111^In-DTPA-A20FMDV2) for in vivo imaging of α_v_β_6_-positive tumors.

### Related Resource Links:

- Chapters in MICAD (knot peptide (http://www.ncbi.nlm.nih.gov/books?term=knot%20AND%20micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D), A20FMDV2 (http://www.ncbi.nlm.nih.gov/books?term=A20FMDV2%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_6_ integrin (http://www.ncbi.nlm.nih.gov/gene/3694))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_6_ integrin (http://www.ncbi.nlm.nih.gov/omim/147558))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A20FMDV2%20and%20synthesis)]

DTPA-NAVPNLRGDLQVLAQKVART (DTPA-A20FMDV2) was prepared with solid-phase peptide synthesis, with the addition of DTPA at the N-terminus (18). A mixture of 1–30 MBq (0.027–0.81 mCi) ^111^InCl_3_ and DTPA-A20FMDV2 was incubated in ammonium acetate buffer (pH 5.5) for 30 min at room temperature. ^111^In-DTPA-A20FMDV2 was found to have a radiochemical purity of >98%. The specific activity of ^111^In-DTPA-A20FMDV2 was not reported. ^111^In-DTPA-A20FMDV2 remained >95% intact after incubation in phosphate-buffered saline for 24 h at 37°C, but it remained only 50% intact in mouse serum for 4 h at 37°C.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A20FMDV2%20and%20%28in%20vitro%20or%20cell%29)]

A receptor-binding assay with biotinylated A20FMDV2 using human A375Ppuro (α_v_β_6_-negative) and A375Pβ6 (α_v_β_6_-positive) cell lines was analyzed with flow cytometry (18). α_5_β_1_, α_v_β_3_, α_v_β_5_, and α_v_β_8_ integrins were present on both cell lines. A20FMDV2 bound well at 1–10,000 nM to A375Pβ6 cells but not to A375Ppuro cells, suggesting that A20FMDV2 is highly selective for α_v_β_6_. DTPA-A20FMDV showed similar binding to these cells as A20FMDV2. Saturation binding assays of ^111^In-DTPA-A20FMDV2 with A375Pβ6 cells exhibited an affinity constant (K_d_) of 1.73 ± 0.46 nM. Internalization assays showed that 50% of total bound radioactivity internalized into A375Pβ6 cells within 20 min and reached 89%–96% by 60 min. On the other hand, neither binding nor internalization was observed in A375Ppuro cells. Confocal microscopy showed binding of A20FMDV2 to the cell membrane of A375Pβ6 cells initially, and most of the peptide was internalized into the cytoplasm by 30 min.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A20FMDV2%20and%20rodentia)]

Saha et al. (18) performed ex vivo biodistribution studies with 1 MBq (0.027 mCi) ^111^In-DTPA-A20FMDV2 in nude mice (n = 3/group) bearing A375Ppuro and A375Pβ6 xenografts on opposite flanks in the shoulder region at 1 h after injection. ^111^In-DTPA-A20FMDV2 exhibited tumor accumulation of 2.1% injected dose (ID)/g in A375Pβ6 tumors at 1 h and only 0.3% ID/g in A375Ppuro tumors. The highest radioactive concentration was found in the kidneys (98% ID/g), followed by the intestine (2.2% ID/g), gallbladder (1.7% ID/g), lung (1.3% ID/g), and stomach (1.2% ID/g). The spleen, muscle, blood, and liver showed low levels of radioactivity (<0.3% ID/g). Co-injection of 100-fold excess DTPA-A20FMDV2 markedly inhibited accumulation of radioactivity by ~70% in the α_v_β_6_-positive tissues, such as the intestine, stomach gallbladder, and A375Pβ6 tumors, but there was little inhibition in the α_v_β_6_-negative tissues, such as the spleen, liver, and A375Ppuro tumors. There was ~50% inhibition in the kidney, but this was determined to be non-specific because 100-fold excess of the non-labeled scrambled peptide (DTPA-A20FMDV2ran) showed similar inhibition in the kidney, with no inhibition in other tissues or in either tumor.

SPECT/computed tomography imaging was performed in nude mice bearing both A375Ppuro and A375Pβ6 xenografts at 1 h after injection of 10–20 MBq (0.27–0.54 mCi) ^111^In-DTPA-A20FMDV2 (18). The kidneys, urinary bladder, intestine, and A375Pβ6 tumors were clearly visualized, whereas little radioactivity was observed in the A375Ppuro tumors. SPECT imaging studies were also performed in nude mice bearing human breast carcinoma cells (MCF10A.DCIS.COM and MCF10A.CA1a) with endogenous expressed α_v_β_6_ integrin. The tumors were clearly visualized with >2% ID/g. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A20FMDV2%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A20FMDV2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A20FMDV2%20and%20%28human%20not%20cell%29)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Breuss J.M., Gallo J., DeLisser H.M., Klimanskaya I.V., Folkesson H.G., Pittet J.F., Nishimura S.L., Aldape K., Landers D.V., Carpenter W., et al. (1995). Expression of the beta 6 integrin subunit in development, neoplasia and tissue repair suggests a role in epithelial remodeling. J Cell Sci.
12 Thomas G.J., Nystrom M.L., Marshall J.F. (2006). Alphavbeta6 integrin in wound healing and cancer of the oral cavity. J Oral Pathol Med.
13 Kawashima A., Tsugawa S., Boku A., Kobayashi M., Minamoto T., Nakanishi I., Oda Y. (2003). Expression of alphav integrin family in gastric carcinomas: increased alphavbeta6 is associated with lymph node metastasis. Pathol Res Pract.
14 Bates R.C. (2005). The alphaVbeta6 integrin as a novel molecular target for colorectal cancer. Future Oncol.
15 DiCara D., Rapisarda C., Sutcliffe J.L., Violette S.M., Weinreb P.H., Hart I.R., Howard M.J., Marshall J.F. (2007). Structure-function analysis of Arg-Gly-Asp helix motifs in alpha v beta 6 integrin ligands. J Biol Chem.
16 Kraft S., Diefenbach B., Mehta R., Jonczyk A., Luckenbach G.A., Goodman S.L. (1999). Definition of an unexpected ligand recognition motif for alphav beta6 integrin. J Biol Chem.
17 Hausner S.H., DiCara D., Marik J., Marshall J.F., Sutcliffe J.L. (2007). Use of a peptide derived from foot-and-mouth disease virus for the noninvasive imaging of human cancer: generation and evaluation of 4-[18F]fluorobenzoyl A20FMDV2 for in vivo imaging of integrin alphavbeta6 expression with positron emission tomography. Cancer Res.
18 Saha A., Ellison D., Thomas G.J., Vallath S., Mather S.J., Hart I.R., Marshall J.F. (2010). High-resolution in vivo imaging of breast cancer by targeting the pro-invasive integrin alphavbeta6. J Pathol.